# ^111^In-Labeled-TNYLFSPNGPIARAW (TNYL-RAW)-polyethylene glycol–coated core-cross-linked polymeric micelle-Cy7

Chemical name: | ^111^In-Labeled-TNYLFSPNGPIARAW (TNYL-RAW)-polyethylene glycol–coated core-cross-linked polymeric micelle-Cy7
Abbreviated name: | ^111^In-TNYL-RAW-CCPM
Synonym:
Agent category: | Peptide
Target: | Ephrin receptor B4 (EphB4)
Target category: | Receptor
Method of detection: | Multimodality imaging: SPECT, planar gamma imaging; optical near-infrared (NIR) fluorescence imaging
Source of signal: | ^111^In, Cy7
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNYL-RAW)]

The ephrin (Eph) receptors constitute the largest member of the receptor tyrosine kinase family (1, 2). The Eph receptors and their ligands (ephrins) mediate numerous biological processes in normal development, particularly in the nervous and cardiovascular systems (3-5). Based on their structures and sequence relationships, ephrins are divided into the ephrin-A class, which are anchored to the cell membrane by a glycosylphosphatidylinositol linkage, and the ephrin-B class, which are transmembrane proteins. The Eph family of receptors is divided into two groups, EphA and EphB, on the basis of the similarity of their extracellular domain sequences and their affinities for binding ephrin-A and ephrin-B ligands. The Eph receptors transmit forward signals via their kinase domain and reverse signals via their transmembrane ephrin ligands (6). EphB–ephrin-B interactions are capable of mediating bi-directional signaling events upon cell–cell contact, either into the receptor-expressing cell as "forward signaling" or into the ligand-expressing cell as "reverse signaling" (7).

Ephrin-2 is expressed on arterial and activated endothelial cells, whereas EphB4 is normally expressed on venous endothelial cells and various blood cells (8). EphB4 selectively binds to ephrin-2 to promote cell signaling and angiogenesis. EphB4 has been implicated in cancer progression and in pathological forms of angiogenesis. Overexpression of EphB4 has been observed in cancer cells and is associated with tumorigenesis via forward signaling and angiogenesis via reverse signaling through ephrin-2 interaction (9). EphB4 forward signaling stimulates cellular proliferation. Koolpe et al. (10) identified a 15-mer peptide, Tyr-Asn-Tyr-Leu-Phe-Ser-Pro-Asn-Gly-Pro-Ile-Ala-Arg-Ala-Trp (TNYL-RAW), to be a selective antagonist of EphB4 using phage display screening. Xiong et al. (11) reported the development of ^64^Cu-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-TNYL-RAW (^64^Cu-DOTA-TNYL-RAW) for positron emission tomography (PET) imaging of EphB4 in nude mice bearing tumor xenografts. Zhang et al. (12) conjugated TNYL-RAW to polyethylene glycol–coated core-cross-linked polymeric micelles (CCPMs) labeled with Cy7 and ^111^In (^111^In-TNYL-RAW-CCPM) for multimodality detection of EphB4 in tumors.

### Related Resource Links:

- Chapters in MICAD (EphB4 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=EphB4+AND+micad%5Bbook%5D))
- Gene information in NCBI (EphB4 (http://www.ncbi.nlm.nih.gov/gene?term=2050), ephrin-B2 (http://www.ncbi.nlm.nih.gov/gene/1948))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EphB4 (http://www.ncbi.nlm.nih.gov/omim/600011), ephrin-B2 (http://www.ncbi.nlm.nih.gov/omim/600527))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNYL-RAW+synthesis)]

CCPM nanoparticles were obtained from Carestream Health (Rochester, NY) (12). There were ~21 Cy7 dye molecules, 180 amino groups, and 19 DTPA moieties per CCPM nanoparticle. Ac-Cys-TNYL-RAW was conjugated to the maleimide-CCPM by sulfhydryl-maleimide bonding. TNYL-RAW-CCPM nanoparticles were purified with column chromatography. The average hydrodynamic diameter of TNYL-RAW-CCPMs was determined to be ~23 nm. There were 60 TNYL-RAW peptides per nanoparticle. The maximum excitation and emission intensities were 755 nm and 781 nm, respectively. ^111^In-TNYL-RAW-CCPM nanoparticles were prepared by incubation of TNYL-RAW-CCPM with ^111^InCl_3_ in sodium acetate buffer (pH 5.2) for 30 min at room temperature with a labeling efficiency of >98%. The specific activity was 180 MBq/nmol (4.9 mCi/nmol). Control ^111^In-CCPM nanoparticles without TNYL-RAW were prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW%20in+vitro)]

Zhang et al. (12) performed binding experiments with TNYL-RAW-CCPM and CCPM using a Biacore sensor chip immobilized with EphB4-Fc. There were increasing amounts of TNYL-RAW-CCPM bound in a dose-dependent manner (0.16–20 nM). The binding kinetics of TNYL-RAW-CCPM to EphB4 is complex due to multi-valency interactions. No binding to EphB4 was detected with CCPM. In vitro binding of TNYL-RAW-CCPM to PC-3M human prostate cancer cells (EphB4-expressing) and A549 human lung adenocarcinoma cells (EphB4-negative) was determined with fluorescence microscopy. PC-3M cells, but not A549 cells, were readily stained with TNYL-RAW-CCPM. The binding of TNYL-RAW-CCPM to PC-3M cells was almost completely blocked by co-incubation with 100-fold excess TNYL-RAW. ^111^In-TNYL-RAW-CCPM exhibited high cellular uptake (cell/medium ratio = 170) in PC-3M cells but not in A549 cells after 15 min of incubation. Incubation with 100-fold excess of TNYL-RAW almost completely inhibited the radioactivity in PC-3M.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+rodentia)]

Zhang et al. (12) performed single-photon emission computed tomography and optical imaging studies in nude mice bearing PC-3M (n = 6/group) and A549 (n = 5/group) tumors at 24 h after injection of 9 MBq (0.24 mCi) (1 × 10^14^ nanoparticles) ^111^In-TNYL-RAW-CCPM or ^111^In-CCPM. PC-3M tumors were clearly visualized, whereas little signal was detected in A549 tumors, with both imaging modalities at 24 h after injection of ^111^In-TNYL-RAW-CCPM. There was little signal detected in PC-3M tumors with ^111^In-CCPM. Co-injection of excess TNYL-RAW reduced the signal to background levels in PC-3M tumors. Ex vivo tumor accumulation was 2.87% injected dose (ID/g) for PC-3M tumors and 1.37% ID/g for A549 tumors at 24 h after injection of ^111^In-TNYL-RAW-CCPM (P< 0.01). Accumulation in the liver and spleen was ~7-fold higher than in the tumors. Tumor/blood ratios were 6.5 and 2.3 for PC-3M and A549 tumors, respectively. Co-injection of excess TNYL-RAW inhibited the tumor/blood ratio of PC-3M tumors to 2.6 (P< 0.01). Accumulation of ^111^In-TNYL-RAW-CCPM (2.87% ID/g) in PC-3M tumors was significantly higher than accumulation of ^111^In-CCPM (1.61% ID/g) or ^64^Cu-DOTA-TNYL-RAW (0.84% ID/g) (P< 0.01). Autoradiography and optical imaging of PC-3M tumor sections showed the localization of both radioactivity and fluorescence signal from ^111^In-TNYL-RAW-CCPM correlated with expression of EphB4. Immunochemical analysis showed high EpB4 expression in PC-3M tumor cells but not in A549 tumor cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20TNYL-RAW+human)]

No publication is currently available.

## References

1 Dodelet V.C., Pasquale E.B. (2000). Eph receptors and ephrin ligands: embryogenesis to tumorigenesis. Oncogene.
2 Pasquale E.B. (1997). The Eph family of receptors. Curr Opin Cell Biol.
3 Adams R.H., Klein R. (2000). Eph receptors and ephrin ligands. essential mediators of vascular development. Trends Cardiovasc Med.
4 Cheng N., Brantley D.M., Chen J. (2002). The ephrins and Eph receptors in angiogenesis. Cytokine Growth Factor Rev.
5 Murai K.K., Pasquale E.B. (2011). Eph receptors and ephrins in neuron-astrocyte communication at synapses. Glia.
6 Noren N.K., Lu M., Freeman A.L., Koolpe M., Pasquale E.B. (2004). Interplay between EphB4 on tumor cells and vascular ephrin-B2 regulates tumor growth. Proc Natl Acad Sci U S A.
7 Pasquale E.B. (2010). Eph receptors and ephrins in cancer: bidirectional signalling and beyond. Nat Rev Cancer.
8 Pfaff D., Heroult M., Riedel M., Reiss Y., Kirmse R., Ludwig T., Korff T., Hecker M., Augustin H.G. (2008). Involvement of endothelial ephrin-B2 in adhesion and transmigration of EphB-receptor-expressing monocytes. J Cell Sci.
9 Noren N.K., Pasquale E.B. (2007). Paradoxes of the EphB4 receptor in cancer. Cancer Res.
10 Koolpe M., Burgess R., Dail M., Pasquale E.B. (2005). EphB receptor-binding peptides identified by phage display enable design of an antagonist with ephrin-like affinity. J Biol Chem.
11 Xiong C., Huang M., Zhang R., Song S., Lu W., Flores L., Gelovani J., Li C. (2011). In vivo small-animal PET/CT of EphB4 receptors using 64Cu-labeled peptide. J Nucl Med.
12 Zhang R., Xiong C., Huang M., Zhou M., Huang Q., Wen X., Liang D., Li C. (2011). Peptide-conjugated polymeric micellar nanoparticles for Dual SPECT and optical imaging of EphB4 receptors in prostate cancer xenografts. Biomaterials.